# [O-^11^C-methyl]4-N-(3-Bromoanilino)-6,7-dimethoxyquinazoline

Chemical name: | [O-^11^C-methyl]4-N-(3-Bromoanilino)-6,7-dimethoxyquinazoline
Abbreviated name: | [^11^C]PD153035, [O-^11^C-methyl]PD153035
Synonym:
Agent category: | Compound
Target: | Epidermal growth factor receptor (EGFR, HER1/erbB-1)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PD153035)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Centuximab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant EGFR with an affinity constant (K_d_) of 0.1 nM. Centuximab is approved for clinical use to treat advanced colorectal cancer patients with metastases by the United States Food and Drug Administration. It is also under investigation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=Erbitux) for treatment of cancers. ^111^In-Cetuximab, ^99m^Tc-cetuximab, and ^68^Cu-cetuximab have been developed for imaging human breast cancer (11-13). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. A novel small molecule, 4-N-(3-bromoanilino)-6,7-dimethoxyquinazoline (PD153035), has been reported to be a potent tyrosine kinase inhibitor preventing EGFR activation and thus inhibiting proliferation of cancer cells (14). PD153035 reversibly binds to the inner membrane ATP-binding domain on EGFR. [^11^C]PD153035 has been evaluated in vivo as a positron emission tomography (PET) agent to measure EGFR expression in tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PD153035+synthesis)]

Fredriksson et al. (15) reported the synthesis of [^11^C]PD153035 by O-methylation of the desmethyl PD153035 precursor with[^11^C]methyl iodide in the presence of NaOH. The mixture was heated for 5 min at 70°C, and [^11^C]PD153035 was purified with high-performance liquid chromatography. The average radiochemical yield was ~30%. The radiochemical purity was >98% with the specific activities of 17-37 GBq/µmol (0.46-1.0 Ci/µmol) at 1-5 min after end of synthesis. The total synthesis time was 45-50 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PD153035%20and%20in%20vitro)]

Fry et al. (16) reported that PD153035 exhibited the inhibition constant (K_i_) of 5 pM for the EGFR and the inhibition concentration 50% (IC_50_) of 29 pM for the tyrosine kinase enzyme. Wang et al. (17) showed that [^11^C]PD153035 accumulation in three cancer cell lines with high (MDA-MB-468), moderate (A-549) and low (MDA-MB-231) expression of EGFR correlated with their EGFR expression levels with [^11^C]PD153035 accumulation of 0.102, 0.052, and 0.038% dose/10^6^ cells after incubation for 60 min, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PD153035%20and%20rodentia)]

Wang et al. (17) performed ex vivo biodistribution studies of [^11^C]PD153035 in nude mice (n = 5/group) bearing MDA-MB-468, A-549 or MDA-MB-231 xenografts. The accumulation in percent injected dose per gram (% ID/g) of the tracer was the highest in the liver (8-11), followed by the intestine (3-5), heart (1, 2), kidney (1, 2), lung (1, 2) and muscle (0.6-0.7) at 10 min after injection. The tracer accumulation in the tumors was 0.65 ± 0.14, 0.30 ± 0.05, 0.22 ± 0.07% ID/g at 30 min for the MDA-MB-468, A-549 or MDA-MB-231 tumors, respectively. Tumor/blood ratios were 8.38, 6.20, and 4.40, respectively. [^11^C]PD153035 radioactivity levels in the three tumors were reduced to background levels by pretreatment with PD153035 (80 mg/kg, 10 min). [^11^C]PD153035 accumulation in the tumors was correlation with the EGFR expression (r^2^ = 0.63, P = 0.003) of the tumor cell lines with immunohistochemical staining.

Fredriksson et al. (15) performed an initial [^11^C]PD153035 PET studies with rats (n = 6) bearing SH-SYS5 neuroblastoma implants showing substantial tumor accumulation with uptake in the liver and intestine in within the 10 min of imaging. The radioactivity level in the tumors gradually decreased with time. Wang et al. (17) performed PET studies of [^11^C]PD153035 in nude mice (n = 6/group) bearing MDA-MB-468, A-549 or MDA-MB-231 xenografts. The three tumors were visualized within 10 min of imaging, followed by a gradual decline of radioactivity. Maximal tumor/muscle ratios were reached within 40-50 min after injection and correlated with the degrees of EGFR expression in the tumor cell lines (r^2^ = 0.65, P = 0.004) and tumor tissue sections (r^2^ = 0.63, P = 0.003).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PD153035%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PD153035%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PD153035%20and%20human)]

Liu et al. (18) performed radiation dosimetry studies with PET scans for 90 min after injection of 329.3 ± 77.8 MBq (8.9 ± 2.1 mCi) of [^11^C] PD153035 in 9 healthy subjects. The renal and hepatobiliary systems were responsible for the excretion of ~23% and ~19% of ID, respectively. The highest absorbed doses were in the urinary bladder wall (60.8 ± 18.5 µGy/MBq), gallbladder wall (24.0 ± 8.01 µGy/MBq), kidneys (14.2 ± 6.36 µGy/MBq), and liver (9.10 ± 1.65 µGy/MBq). The effective dose was 7.43 ± 1.10 µSv/MBq. Radioactivity accumulation in the lungs, spleen, brain, bone marrow, and muscles was low.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Ping Li W., Meyer L.A., Capretto D.A., Sherman C.D., Anderson C.J. (2008). Receptor-binding, biodistribution, and metabolism studies of 64Cu-DOTA-cetuximab, a PET-imaging agent for epidermal growth-factor receptor-positive tumors. Cancer Biother Radiopharm.
12 Milenic D.E., Wong K.J., Baidoo K.E., Ray G.L., Garmestani K., Williams M., Brechbiel M.W. (2008). Cetuximab: preclinical evaluation of a monoclonal antibody targeting EGFR for radioimmunodiagnostic and radioimmunotherapeutic applications. Cancer Biother Radiopharm.
13 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
14 Bos M., Mendelsohn J., Kim Y.M., Albanell J., Fry D.W., Baselga J. (1997). PD153035, a tyrosine kinase inhibitor, prevents epidermal growth factor receptor activation and inhibits growth of cancer cells in a receptor number-dependent manner. Clin Cancer Res.
15 Fredriksson A., Johnstrom P., Thorell J.O., von Heijne G., Hassan M., Eksborg S., Kogner P., Borgstrom P., Ingvar M., Stone-Elander S. (1999). In vivo evaluation of the biodistribution of 11C-labeled PD153035 in rats without and with neuroblastoma implants. Life Sci.
16 Fry D.W., McMichael A., Singh J., Dobrusin E.M., McNamara D.J. (1994). Design of a potent peptide inhibitor of the epidermal growth factor receptor tyrosine kinase utilizing sequences based on the natural phosphorylation sites of phospholipase C-gamma 1. Peptides.
17 Wang H., Yu J.M., Yang G.R., Song X.R., Sun X.R., Zhao S.Q., Wang X.W., Zhao W. (2007). Further characterization of the epidermal growth factor receptor ligand 11C-PD153035. Chin Med J (Engl).
18 Liu N., Li M., Li X., Meng X., Yang G., Zhao S., Yang Y., Ma L., Fu Z., Yu J. (2009). PET-based biodistribution and radiation dosimetry of epidermal growth factor receptor-selective tracer 11C-PD153035 in humans. J Nucl Med.